# Al^18^F-1,4,7-Triazacyclononane,1-glutaric acid-4,7-acetic acid-Glu-[cyclo(Arg-Gly-Asp-D-Phe-Lys)]_2_

Chemical name: | Al^18^F-1,4,7-Triazacyclononane,1-glutaric acid-4,7-acetic acid-Glu-[cyclo(Arg-Gly-Asp-D-Phe-Lys)]_2_
Abbreviated name: | Al^18^F-NODAGA-E-[c(RGDfK)]_2_
Synonym:
Agent category: | Peptide
Target: | Integrin α_v_β_3_
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=23831237), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=56237028) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=3678&ordinalpos=5&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about integrin α_v_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA%20c(RGDfK))]

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (1). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (2-7). Expression of the α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. Antagonists of α_v_β_3_ are being studied as antitumor and antiangiogenic agents, and the agonists of α_v_β_3_ are being studied as angiogenic agents for coronary angiogenesis (6, 8, 9). Extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) contain a tripeptide sequence consisting of Arg-Gly-Asp (RGD), which binds to a variety of integrins, including α_v_β_3_. Various radiolabeled antagonists have been introduced for use with the imaging of tumors and tumor angiogenesis (10).

Most cyclic RGD peptides are composed of five amino acids. Haubner et al. (11) reported that various cyclic RGD (c(RGD)) peptides exhibit selective inhibition of binding to α_v_β_3_ (inhibition concentration (IC_50_), 7–40 nM) but not to integrins α_v_β_5_ (IC_50_, 600–4,000 nM) or α_IIb_β_3_ (IC_50_, 700–5,000 nM). Various radiolabeled c(RGD) peptides have been found to have high accumulation in tumors in nude mice (12). Dijkgraaf et al. (13) reported the evaluation of Al^18^F-1,4,7-triazacyclononane,1-glutaric acid-4,7-acetic acid-Glu-[cyclo(Arg-Gly-Asp-D-Phe-Lys)]_2_ (Al^18^F-NODAGA-E-[c(RGDfK)]_2_) for use with positron emission tomography (PET) imaging of α_v_β_3_ in tumors.

### Related Resource Links:

- Chapters in MICAD (RGD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=RGD+AND+micad%5Bbook%5D))
- Gene information in NCBI (α_v_ integrin (http://www.ncbi.nlm.nih.gov/gene/3685), β_3_ integrin (http://www.ncbi.nlm.nih.gov/gene/3690))
- Articles in Online Mendelian Inheritance in Man (OMIM) (α_v_ integrin (http://www.ncbi.nlm.nih.gov/omim/193210), β_3_ integrin (http://www.ncbi.nlm.nih.gov/omim/173470))
- Clinical trials (RGD (http://www.clinicaltrials.gov/ct2/results?term=RGD))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA%20c(RGDfK)+synthesis)]

Dijkgraaf et al. (13) prepared the synthesis of Al^18^F-NODAGA-E-[c(RGDfK)]_2_ by reacting NODAGA-E-[c(RGDfK)]_2_ with Al^18^F in sodium acetate buffer (pH ~4.1) for 15 min at 100°C. Radiochemical purity was >98% as determined with high-performance liquid chromatography, with an overall yield of 20%. The specific activity was 1.8 MBq/nmol (0.049 mCi/nmol) at the end of synthesis. The total synthesis time was <45 min. Al^18^F-NODAGA-E-[c(RGDfK)]_2_ had a logP value of −4.26 ± 0.02.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA%20c(RGDfK)+in+vitro)]

Dijkgraaf et al. (13) performed in vitro solid-phase binding assays of ^111^In-DOTA-E-[c(RGDfK)]_2_ with human α_v_β_3_ integrin. NODAGA-E-[c(RGDfK)]_2_ had an IC_50_ value of 0.043 ± 0.037 nM. DOTA-E-[c(RGDfK)]_2_ had an IC_50_ value of 0.037 ± 0.085 nM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA%20c(RGDfK)+rodentia)]

Dijkgraaf et al. (13) performed ex vivo biodistribution studies of 0.4 MBq (11 µCi) Al^18^F-NODAGA-E-[c(RGDfK)]_2_ with nude mice (n = 3–5/group) bearing SK-RC-52 human renal carcinoma tumors at 2 h after injection. The tumor accumulation was 3.4 ± 0.2% injected dose/gram (ID/g). The organ with the highest accumulation was the kidney (3.1% ID/g), followed by the intestine (2.8% ID/g), liver (1.5% ID/g), and spleen (1.5% ID/g). Low accumulation (<1% ID/g) was observed in the muscle, heart, lung, stomach, pancreas, and femur. Very low radioactivity was detected in blood (<0.1% ID/g). Coinjection of excess NODAGA-E-[c(RGDfK)]_2_ resulted in 75% reduction of radioactivity in the tumor (P < 0.001). The accumulation was also reduced in the liver, lung, intestine, stomach, femur, and spleen (this may be partly mediated by α_v_β_3_ integrin in these tissues), but the kidney was not affected. PET scans showed that the tumor was clearly visualized at 2 h after injection of 10 MBq (0.27 mCi) Al^18^F-NODAGA-E-[c(RGDfK)]_2_. Some accumulation was observed in the kidneys. Coinjection of excess NODAGA-E-[c(RGDfK)]_2_ reduced radioactivity in the tumor but not in the kidneys. Similar findings of ex vivo and PET imaging studies were obtained with ^68^Ga-NODAGA-E-[c(RGDfK)]_2_. The ex vivo radioactivity levels of ^68^Ga-NODAGA-E-[c(RGDfK)]_2_ in the tumor (6.3 ± 0.8% ID/g) and intestine (~5.0% ID/g) were higher than those of Al^18^F-NODAGA-E-[c(RGDfK)]_2_ (3.4 ± 0.2% ID/g and 2.8% ID/g, respectively).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA%20c(RGDfK)+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA%20c(RGDfK)+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=NODAGA%20c(RGDfK)+human)]

No publication is currently available.

## References

1 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
4 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
5 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
6 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
7 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
8 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
9 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
10 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
11 Haubner R., Wester H.J., Burkhart F., Senekowitsch-Schmidtke R., Weber W., Goodman S.L., Kessler H., Schwaiger M. (2001). Glycosylated RGD-containing peptides: tracer for tumor targeting and angiogenesis imaging with improved biokinetics. J Nucl Med.
12 Chen X., Park R., Shahinian A.H., Tohme M., Khankaldyyan V., Bozorgzadeh M.H., Bading J.R., Moats R., Laug W.E., Conti P.S. (2004). 18F-labeled RGD peptide: initial evaluation for imaging brain tumor angiogenesis. Nucl Med Biol.
13 Dijkgraaf I., Terry S.Y., McBride W.J., Goldenberg D.M., Laverman P., Franssen G.M., Oyen W.J., Boerman O.C. (2013). Imaging integrin alpha-v-beta-3 expression in tumors with an (18) F-labeled dimeric RGD peptide. Contrast Media Mol Imaging.